# 5-Carboxy-fluorescein-labeled octreotate

Chemical name: | 5-Carboxy-fluorescein-labeled octreotate
Abbreviated name: | OcF
Synonym:
Agent Category: | Polypeptides
Target: | Somatostatin receptors (SSTRs)
Target Category: | Receptors
Method of detection: | Optical imaging (miniaturized confocal laser-scanning fluorescence microscopy)
Source of signal / contrast: | 5-Carboxy-fluorescein
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=confocal+laser+scanning+microscopy+and+in+vivo+and+molecular+imaging)]

Octreotate labeled with 5-carboxy-fluorescein, abbreviated as OcF, is an optical imaging agent developed by Fottner et al. for in vivo imaging of somatostatin receptors (SSTRs) in neuroendocrine tumors with miniaturized confocal laser-scanning microscopy (CLM) (1). SSTRs are highly expressed in neuroendocrine tumors (2, 3). The excitation and emission wavelengths of 5-carboxy-fluorescein are 492 nm and 518 nm, respectively. The molecular weight of octreotate is 1033.3.

CLM is an emerging technique that integrates the miniaturized components of a confocal laser scanner into the tip of a conventional endoscope (4-7). During imaging, a solid laser delivers an excitation wavelength of 488 nm on the surface of target organs, and light emission is detected at 505–585 nm. Serial images are collected at a scan rate of 0.8 frames/s at 1024 × 1024 pixels or 1.6 frames/s at 1024 × 512 pixels. The laser power output can be adjusted from 0 µW to 1000 µW to achieve appropriate tissue contrast. The optical slice thickness is usually 7 μm, with a lateral resolution of 0.7 μm and an imaging plane depth to 250 μm from the tissue surface. Tissue images are produced on the basis of different refractive indices from biological tissues, and image contrast is enhanced with application of contrast agents such as intravenous sodium fluorescein or topical acriflavine (7, 8). Virtual histology can be created with CLM, which allows visualization of pathological changes at cellular and subcellular levels in addition to standard videoendoscopy (5, 7). Studies with CLM have demonstrated its effectiveness in screening inflammatory and early malignant diseases of the gastrointestinal tract (1). However, the CLM technique does not allow clear, simultaneous, in vivo imaging of the tissue anatomy together with a dynamic visualization of molecular targets like the SSTRs (1).

Fottner et al. developed a miniaturized CLM technique that allows the specific molecular imaging of SSTRs in vivo and in real time (1). For selective visualization of SSTRs, a contrast agent for CLM was specifically synthesized by conjugating 5-carboxy-fluorescein to octreotate (referred to as OcF). With the miniaturized CLM and OcF, equal morphological resolution of SSTR-expressing cell structures (pancreatic islet cells, renal tubular cells, and neuroendocrine tumors) was achieved, unlike with standard histological tissue investigation. Fottner et al. concluded that the CLM technique together with OcF allows specific visualization of SSTR-expressing neuroendocrine tumor cells, while expression of SSTRs and SSTR-mediated endocytosis of somatostatin and its analogs in neuroendocrine tumors represent the molecular basis for various clinical diagnostic and therapeutic applications (1).

### Related Resource Links:

- MICAD chapters on SSTR imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=somatostatin+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on SSTRs (http://www.ncbi.nlm.nih.gov/gene/?term=somatostatin+receptors)
- Articles of SSTRs in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=somatostatin%20receptors)
- Somatostatin analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance)
- Bioassays of SSTRs in PubChem (http://www.ncbi.nlm.nih.gov/pcassay?term=somatostatin%20receptors)
- SSTR-related clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptors)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20233796)]

Fottner et al. synthesized OcF with Fmoc solid-phase peptide synthesis and labeled the peptide with 5-carboxy-fluorescein on solid phase (1). The labeled product (OcF) was cleaved from resin and purified. The purity of OcF was >99%. The labeling efficiency and the number of fluorescein molecules per octreotate were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20233796)]

The affinity of OcF to SSTRs was tested against ^125^I-Tyr3–labeled octreotide with a membrane preparation from rat cerebral cortex (predominantly expressing SSTR subtype 2 (SSTR2)) (1). The 50% inhibitory concentration (IC_50_) of OcF was 6.2 nmol, which was comparable to the IC_50_ values of [^111^In-DTPA]octreotide and [^90^Y-DOTA-Tyr]octreotide (22 nmol and 11 nmol, respectively). [^111^In-DTPA]octreotide and [^90^Y-DOTA-Tyr]octreotide are currently used for clinical imaging purposes (2, 3, 9).

The biological activity of OcF was evaluated after incubation with AR42J and Panc1 cells (1). AR42J is a rat pancreatic cancer cell line with abundant expression of SSTR2–SSTR5, with SSTR2 being the predominant subtype. Panc1 is a human pancreatic adenocarcinoma cell line with barely detectable expression of SSTRs. Unlabeled octreotide resulted in a >50% suppression of the AR42J cell proliferation at 5 µmol, whereas OcF had similar activity only at >100 µmol. However, both agents had a similar maximum antiproliferative effect at 250 µmol. The results suggested that OcF had a comparable maximal antiproliferative effect at higher but still physiological concentrations. In SSTR-negative Panc1 cells, none of the unlabeled octreotide and OcF had any antiproliferative effect.

In vitro SSTR imaging was performed with conventional fluorescence and confocal microscopy (1). Time- and dose-dependent staining of the AR42J cells was observed with a maximum intensity at 100 µmol and a still detectable contrast at 0.1 µmol OcF. Best contrast was achieved at a concentration of 10 µmol OcF after incubation for 30 min. Similar results were obtained when the miniaturized CLM was applied. Cell staining with OcF was blocked when the cells were pre-incubated with unlabeled octreotide. When SSTR-negative Panc1 tumor cells were used, no fluorescence was observed after incubation with OcF.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20233796)]

In vivo imaging of SSTR-expressing pancreatic islet cells, renal tubular cells, and tumor xenografts was performed with CLM after intravenous injection of OcF (1). The mouse pancreas and kidneys were surgically exposed, and the miniaturized CLM probe was directly placed onto the tissues.

Pancreas imaging showed that a subpopulation of cells started to exhibit contrast at the cell surface 15 min after OcF injection. Internalization and cytoplasmic distribution were observed after an additional 15–30 min. The bright cells that were clearly contrasted with surrounding tissue represented the SSTR-positive islet cells as confirmed with ex vivo immunohistochemistry (1).

Kidney imaging showed that the tubular cells of the cortex already had weak superficial staining a few minutes after injection, and at 15–30 min had a bright surface staining and the beginning of cytoplasmic distribution. Maximum staining intensity was reached after 30–45 min and gradually attenuated after 60 min, with a bright-contrast enhancement of the renal tubular system after tubular secretion. Not all tubular cells of the renal cortex were contrasted after OcF application, which was in good accordance with ex vivo immunohistochemistry that showed an irregular expression of the SSTR2 in renal tubular cells (1).

In tumor xenograft imaging, SSTR-expressing AR42J tumor cells displayed a bright cell surface and cytoplasmic staining (1). SSTR-Negative Panc1 tumor cells were detectable only by the background fluorescence with twice the amount of OcF. The sensitivity and specificity of the miniaturized CLM with OcF for detection of SSTR-positive cells in vivo were 87.5% and 100%, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Fottner C., Mettler E., Goetz M., Schirrmacher E., Anlauf M., Strand D., Schirrmacher R., Kloppel G., Delaney P., Schreckenberger M., Galle P.R., Neurath M.F., Kiesslich R., Weber M.M. (2010). In vivo molecular imaging of somatostatin receptors in pancreatic islet cells and neuroendocrine tumors by miniaturized confocal laser-scanning fluorescence microscopy. Endocrinology.
2 Kwekkeboom D.J., Kam B.L., van Essen M., Teunissen J.J., van Eijck C.H., Valkema R., de Jong M., de Herder W.W., Krenning E.P. (2010). Somatostatin-receptor-based imaging and therapy of gastroenteropancreatic neuroendocrine tumors. Endocr Relat Cancer.
3 Khan I.U., Beck-Sickinger A.G. (2008). Targeted tumor diagnosis and therapy with peptide hormones as radiopharmaceuticals. Anticancer Agents Med Chem.
4 Fricker M.D., Meyer A.J. (2001). Confocal imaging of metabolism in vivo: pitfalls and possibilities. J Exp Bot.
5 Goetz M., Kiesslich R. (2008). Confocal endomicroscopy: in vivo diagnosis of neoplastic lesions of the gastrointestinal tract. Anticancer Res.
6 Goetz M., Kiesslich R. (2010). Advances of endomicroscopy for gastrointestinal physiology and diseases. Am J Physiol Gastrointest Liver Physiol.
7 Kiesslich R., Goetz M., Neurath M.F. (2008). Confocal laser endomicroscopy for gastrointestinal diseases. Gastrointest Endosc Clin N Am.
8 Wessels J.T., Yamauchi K., Hoffman R.M., Wouters F.S. (2010). Advances in cellular, subcellular, and nanoscale imaging in vitro and in vivo. Cytometry A.
9 Kwekkeboom D.J., de Herder W.W., van Eijck C.H., Kam B.L., van Essen M., Teunissen J.J., Krenning E.P. (2010). Peptide receptor radionuclide therapy in patients with gastroenteropancreatic neuroendocrine tumors. Semin Nucl Med.